# ^68^Ga-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-Asp-cyclohexylalanine-Phe-D-Ser-D-Arg-Tyr-Leu-Trp-Ser-NH_2_ (AE105-NH_2_)

Chemical name: | ^68^Ga-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-Asp-cyclohexylalanine-Phe-D-Ser-D-Arg-Tyr-Leu-Trp-Ser-NH_2_ (AE105-NH_2_)
Abbreviated name: | ^68^Ga-NODAGA-AE105-NH_2_, ^68^Ga-NODAGA-D-Cha-F-s-r-Y-L-W-S-NH_2_
Synonym:
Agent category: | Peptide
Target: | Urokinase-type plasminogen activator receptor (uPAR)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=48146021), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=48146020) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=5329) for more information about uPAR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play an important role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degradation of the basement membrane and ECM (3). Several families of proteases are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastasis (4-7).

Urokinase-type plasminogen activator (uPA) is a serine protease (8, 9). The uPA/uPA receptor (uPAR) system is responsible for tissue degradation after plasminogen activation to plasmin, which leads to a cascade of proteolysis or thrombolysis, depending on the physiological conditions. uPA also directly activates MMPs, vascular endothelial growth factor, and human growth factor (10). Malignant tumors often express high levels of uPA and uPAR (11); therefore, the uPA/uPAR system is linked to vascular diseases and cancer. The synthetic peptide Asp-cyclohexylalanine-Phe-D-Ser-D-Arg-Tyr-Leu-Trp-Ser (AE105) has been identified to have a high affinity for human uPAR (dissociation constant (K_d_) = 0.4 nM) (12), and AE105 has been labeled with ^64^Cu (T_1/2_ = 12.7 h, β^+^ = 17.8%) as ^64^Cu-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-AE105 (^64^Cu-DOTA-AE105) and ^64^Cu-DOTA-AE105-NH_2_ for use in positron emission tomography (PET) imaging of uPAR expression in tumors (13, 14). Persson et al. (15) also prepared ^68^Ga-1,4,7-triazacyclononane,1-glutaric acid-4,7-acetic acid-AE105-NH_2_ (^68^Ga-NODAGA-AE105-NH_2_) and ^68^Ga-DOTA-AE105-NH_2_ for evaluation as alternative PET agents (^68^Ga: T_1/2_ = 68 min, β^+^ = 89%).

### Related Resource Links

- Chapters in MICAD (uPAR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=uPAR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (uPAR (http://www.ncbi.nlm.nih.gov/gene/5329), uPA (http://www.ncbi.nlm.nih.gov/gene/5328))
- Articles in Online Mendelian Inheritance in Man (OMIM) (uPAR (http://omim.org/entry/173391), uPA (http://omim.org/entry/191840))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105+synthesis)]

Persson et al. (15) performed NODAGA chelation of the N-terminus of AE105-NH_2_via solid-phase synthesis. A mixture of AE105-NH_2_ and NODAGA-tris(tBu)ester in a molar ratio of 1:3 was incubated for 24–48 h at room temperature. The NODAGA-AE105-NH_2_ conjugate was purified with high-performance liquid chromatography (HPLC). The number of NODAGA molecules per peptide was ~1 as determined with mass spectroscopy. For radiolabeling, NODAGA-AE105-NH_2_ (5 nmol) was added to ^68^GaCl_3_ diluted in 0.1 M sodium acetate buffer (pH 5.0). The reaction mixture was incubated for 15 min at 25ºC. ^68^Ga-NODAGA-AE105-NH_2_ was purified with a Sep-Pak column (>95% radiochemical purity). ^68^Ga-DOTA-AE105-NH_2_ was prepared similarly. The specific activities of ^68^Ga-NODAGA-AE105-NH_2_ and ^68^Ga-DOTA-AE105-NH_2_ were ~20 GBq/μmol (0.54 Ci/μmol) at the end of synthesis. Total synthesis time and yields for both tracers were not reported. The log P values were –1.15 ± 0.1 and –1.75 ± 0.1 for ^68^Ga-NODAGA-AE105-NH_2_ and ^68^Ga-DOTA-AE105-NH_2_, respectively. Both tracers were >98% intact in both saline buffer and mouse plasma for 60 min at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105+and+in+vitro)]

Persson et al. (15) performed binding experiments with AE105-NH_2_, NODAGA-AE105-NH_2_, and DOTA-AE105-NH_2_ with the use of a Biacore sensor chip immobilized with pro-uPA. The IC_50_ values for inhibiting the binding of 0.5 nM uPAR to pro-uPA were 7.6 ± 2.0 nM, 3.4 ± 0.4 nM, and 6.7 ± 0.9 nM for AE105-NH_2_, NODAGA-AE105-NH_2_, and DOTA-AE105-NH_2_, respectively. Cellular accumulation of ^68^Ga-NODAGA-AE105-NH_2_ and ^68^Ga-DOTA-AE105-NH_2_ was assessed by incubating the agents with U87MG human glioblastomas (uPAR-positive) cells for 120 min at 37°C. Both tracers reached a plateau accumulation at 60 min after incubation, with 1.46 ± 0.1% and 1.37 ± 0.1% incubation dose, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105+rodentia)]

Persson et al. (15) performed dynamic PET imaging studies for 60 min after injection of 5–7 MBq (0.135–0.189 mCi, 0.5 nmol) ^68^Ga-NODAGA-AE105-NH_2_ or ^68^Ga-DOTA-AE105-NH_2_ in mice (n = 3/group) bearing U87MG tumors in the left and right flanks. The tumors and kidneys were visualized for both tracers at 10–60 min. Region of interest (ROI) analysis showed that the tumor accumulation values of ^68^Ga-NODAGA-AE105-NH_2_ were 2.5% injected dose per gram (ID/g), 2.0% ID/g, and 2.0% ID/g at 10, 30, and 60 min after injection. The tumor/blood, tumor/muscle, and tumor/liver ratios at 60 min were 1, 5, and 1, respectively. The tumor accumulation values of ^68^Ga-DOTA-AE105-NH_2_ were 2.2% ID/g, 1.3% ID/g, and 1.0% ID/g at 10, 30, and 60 min after injection, respectively. The tumor/blood, tumor/muscle, and tumor/liver ratios at 60 min were 1, 3, and 1, respectively. ^68^Ga-NODAGA-AE105-NH_2_ and ^68^Ga-DOTA-AE105-NH_2_ exhibited lower tumor accumulation and a lower tumor/muscle ratio than ^64^Cu-DOTA-AE105-NH_2_ (4.8% ID/g and 16) at 60 min after injection, as reported previously in the same tumor model. No blocking studies and ex vivo biodistribution studies were performed with either tracer.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105+human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
5 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
6 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
7 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
8 Choong P.F., Nadesapillai A.P. (2003). Urokinase plasminogen activator system: a multifunctional role in tumor progression and metastasis. Clin Orthop Relat Res.
9 Rabbani S.A., Mazar A.P. (2001). The role of the plasminogen activation system in angiogenesis and metastasis. Surg Oncol Clin N Am.
10 Folkman J., Shing Y. (1992). Angiogenesis. J Biol Chem.
11 Duffy M.J., Maguire T.M., McDermott E.W., O'Higgins N. (1999). Urokinase plasminogen activator: a prognostic marker in multiple types of cancer. J Surg Oncol.
12 Ploug M., Ostergaard S., Gardsvoll H., Kovalski K., Holst-Hansen C., Holm A., Ossowski L., Dano K. (2001). Peptide-derived antagonists of the urokinase receptor. affinity maturation by combinatorial chemistry, identification of functional epitopes, and inhibitory effect on cancer cell intravasation. Biochemistry.
13 Li Z.B., Niu G., Wang H., He L., Yang L., Ploug M., Chen X. (2008). Imaging of urokinase-type plasminogen activator receptor expression using a 64Cu-labeled linear peptide antagonist by microPET. Clin Cancer Res.
14 Persson M., Madsen J., Ostergaard S., Jensen M.M., Jorgensen J.T., Juhl K., Lehmann C., Ploug M., Kjaer A. (2012). Quantitative PET of human urokinase-type plasminogen activator receptor with 64Cu-DOTA-AE105: implications for visualizing cancer invasion. J Nucl Med.
15 Persson M., Madsen J., Ostergaard S., Ploug M., Kjaer A. (2012). (68)Ga-labeling and in vivo evaluation of a uPAR binding DOTA- and NODAGA-conjugated peptide for PET imaging of invasive cancers. Nucl Med Biol.